# Near-infrared dye IRDye 800CW-labeled butyrylcholinesterase

Chemical name: | Near-infrared dye IRDye 800CW-labeled butyrylcholinesterase
Abbreviated name: | BChE-IRDye 800CW
Synonym:
Agent Category: | Protein
Target: | Butyrylcholinesterase
Target Category: | Enzyme
Method of detection: | Near-infrared fluorescent optical imaging
Source of signal / contrast: | IRDye 800CW
Activation: | No
Studies: | - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=590&log$=genesensor5&logdbfrom=protein), nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&term=(bche%5bgene%5d)%20AND%20(Homo%20sapiens%5borgn%5d)%20AND%20alive%5bprop%5d%20NOT%20newentry%5bgene%5d&log$=genesensor5&logdbfrom=nuccore&sort=weight), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&term=(bche%5bgene%5d)%20AND%20(Homo%20sapiens%5borgn%5d)%20AND%20alive%5bprop%5d%20NOT%20newentry%5bgene%5d&log$=genesensor5&logdbfrom=nuccore&sort=weight) for more information about butyrylcholinesterase.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase)]

Cholinesterase (ChE) is an enzyme that hydrolyzes the neurotransmitter acetylcholine into choline and acetic acid, and thus shuts off neural transmission (1, 2). There are two types of ChE: acetylcholinesterase (AChE, also known as erythrocyte cholinesterase or acetylcholine acetylhydrolase) and butyrylcholinesterase (BChE or BuChE, also known as plasma cholinesterase, pseudocholinesterase, or acylcholine acylhydrolase) (2). Both enzymes are present in cholinergic and noncholinergic tissues as well as in plasma and other body fluids. They differ in substrate specificity, behavior in excess substrate, and susceptibility to inhibitors.

BChE is encoded by the BCHE gene, which is located in humans on chromosome 3q26.1-q26.2 (3). Mutations of the BCHE gene result in various genotypes and phenotypes (4), and some BCHE gene variants, such as atypical, K, J, and H variants, cause reduced activity of BChE. The silent variants lead to total loss of the enzyme activity (0–2% of normal activity). On the other hand, some variants result in increased activity, such as the C5+ variant (combination of BChE with an unidentified protein), the Cynthiana variant (increased amount of BChE than normal level), and the Johannesburg variant (increased BChE activity with normal enzyme level). In the absence of relaxants, there is no known disadvantage for individuals with these variants.

BChE is synthesized in many tissues, including the liver, lungs, heart, and brain. Similar to AChE, a single BCHE gene gives rise to different protein products by alternative splicing in the coding region of the original transcript. This provides a series of diverse but related molecular forms of BChE (G1, G2, and G4). G4 is the predominant isoform in the mature brain. These forms have similar catalytic properties, but they exhibit different cellular and extracellular distributions and non-catalytic activities.

BChE possesses three different enzymatic activities: esterase, aryl acylamidase, and peptidase. The esterase activity of BChE plays an important role in scavenging anti-AChE compounds such as cocaine, heroin, and organophosphate before they reach AChE at physiologically important sites. In the absence of AChE, BChE is believed to serve as a backup to AChE in supporting and regulating cholinergic transmission (5). BChE also inactivates some drugs, e.g., aspirin, amitriptyline, and bambuterol. The aryl acylamidase activity of BChE may be involved in the crosstalk between seratonergic and cholinergic neurotransmission systems, but it is still poorly understood. The peptidase activity of BChE is related to the development and progress of Alzheimer’s disease (AD) which is characterized by a loss of cholinergic neurons (6). In the brains of patients with AD, the level of the membrane-bound G4 form of AChE is selectively reduced by 90% or more in certain regions, while the level of the G1 form is largely unchanged. On the contrary, the G1 form of BChE shows a 30–60% increase, while the G4 form decreases or remains the same as in the normal brain (7). It has been indicated that BChE, which is found in the neuritic plaques and tangles, cleaves the amyloid precursor protein to the β-amyloid protein and helps β-amyloid diffusion to β-amyloid plaques. Abnormal expressions of BChE and AChE have also been observed in human tumors such as meningioma, glioma, acoustic neurinomas, and lung, colon and ovarian cancers (8). However, the relationship is not clear between altered BChE and AChE expressions and tumorigenesis.

Because of the potential diagnostic and therapeutic values, investigators have synthesized various radiolabeled butyrylcholine analogs and tested their feasibilities as tracers for measurement of cerebral BChE activity (9-12). In an attempt to better understand the real-time distribution of BChE from injection site, Duysen and colleagues labeled the BChE directly with fluorescent dye and investigated the BChE pharmacokinetics in BChE knockout mice (13, 14). There is no detectable BChE activity in all tissues and plasma of the BChE−/− mice.

### AChE- and BChE-Related Resource Links

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=acetylcholinesterase++AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (AChE (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=43&log$=genesensor5&logdbfrom=protein) and BChE (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&term=(bche%5bgene%5d)%20AND%20(Homo%20sapiens%5borgn%5d)%20AND%20alive%5bprop%5d%20NOT%20newentry%5bgene%5d&log$=genesensor5&logdbfrom=nuccore&sort=weight)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=cholinesterase)
- Clinical trials (AChE (http://www.clinicaltrials.gov/ct2/results?term=acetylcholinesterase), BChE (http://www.clinicaltrials.gov/ct2/results?term=butyrylcholinesterase))
- Substances (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=cholinesterase) and Compounds (http://www.ncbi.nlm.nih.gov/pccompound/?term=cholinesterase) in PubChem
- Drug information in FDA (http://google-test.fda.gov/search?q=Cholinesterase+inhibitors&x=9&y=10&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase+and+imaging)]

Lyophilized horse BChE containing 1,440 units of BChE activity (1 unit hydrolyzes 1 µmol butyrylthiocholine per min at 25ºC, pH 7.0, when the butyrylthiocholine concentration is 1 mmol) was labeled with IRDye 800CW following the manufacturer’s instruction (13, 14). The fluorescent dye contains an N-hydroxysuccinimide ester reactive group that coupled with the lysines of BChE protein. The conjugate was dialyzed extensively against phosphate-buffered saline to remove excess unreacted dye. The labeled BChE bound 1 dye molecule per mole of protein and lost 6.7% of its initial activity (13). In another report from the same laboratory, the labeled BChE bound 5 dye molecules per mole of protein and lost 60% of its initial activity (14). The labeled BChE was examined on the nondenaturing gel where the primary tetramers with a molecular weight of 340 kDa were confirmed.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=BChE-IRDye+800CW+and+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=BChE+and%20imaging)]

Duysen et al. analyzed the biodistribution of BChE-IRDye 800CW in BChE knockout (BChE−/−) mice after intramuscular injection of either dye alone (n = 2 mice), BChE-IRDye 800CW (n = 7 mice), or native BChE (n = 3 mice) (14). The genetic background of the BChE−/− mice is strain 129Sv. All tissues and plasma of the BChE−/− mice are devoid of BChE activity (5, 15, 16). BChE−/− mice have no distinguishable phenotype. With in vivo optical imaging, the highest fluorescent intensity was observed at the injection site and in the vasculature, bladder, peritoneal cavity, and liver on day 1 after injection of BChE-IRDye 800CW. On day 3, the signal in the liver and bladder was reduced, while the signal in other organs remained comparable to day 1. On day 7, the fluorescent signal in all examined tissues was reduced but still evident. On day 16, the fluorescence was observable only at the site of injection. With ex vivo imaging of frozen sections of the organs prepared on day 3 after injection, strong fluorescence was observed throughout the liver section, at the injection site, in the cortex and medulla of the kidneys, and in the dense connective tissue of the spleen. Muscle, kidneys, fallopian tubes, and lungs had 5–10% of the intensity in the liver, and the spleen, salivary glands, and heart had 1–2% of the intensity in the liver. Measurement of the plasma BChE activity showed that the half-lives of the native BChE and BChE-IRDye 800CW were 67 h and 30 h, respectively. The maximum plasma activity was detected at 30 h after injection for both native BChE (400 units/ml) and BChE-IRDye 800CW (170 units/ml). On day 12, the plasma activity decreased to 1 unit/ml, a level similar to the 1.9 units/ml in wild-type mice. In most organs examined, the maximum enzyme activity was reached on the first day, and a low level of activity was still detected on day 16 after injection. The BChE-IRDye 800CW was metabolized in the liver and excreted through the kidneys in the same manner as the dye. However, the fluorescent intensities did not correlate with the measured BChE activity levels in organs. The brain was free of fluorescence and BChE enzyme activity, indicating that BChE-IRDye 800CW did not cross the blood–brain barrier.

Johnson et al. investigated the distribution of BChE-IRDye 800CW in the brain of BChE−/− mice (n = 16) after intrathecal injection at the L5–L6 interspace (13). The control mice were injected with IRDye 800CW alone. The fluorescent signal in the mouse brain peaked at 6 h for both BChE-IRDye 800CW and dye alone. At 25 h, the signal in the brains of control mice returned to background levels, while the signal in the brains of mice injected with BChE-IRDye 800CW remained at a level equivalent to that observed at 15 min after injection. With ex vivo imaging of organs dissected at 4 h after injection, intense fluorescence was observed in the brain, spinal column, liver, and kidneys of both control mice and mice injected with BChE-IRDye 800CW (n = 3 mice/group). The highest fluorescent signal was observed in the cistern region (prepontine, magna, and supracerebellar) of the brain. At 25 h after injection, mice treated with BChE-IRDye 800CW (n = 5) still had measurable levels of fluorescent signal in the organs in contrast to the organs from control mice (n = 5), which exhibited no detectable signal. The presence of BChE were confirmed with activity assays. There was no detectable BChE activity in the plasma and brain in the control mice (n = 21) at any time point after injection of dye alone and in the treated mice (n = 8) before injection, while the activity was 42 ± 11 units/ml at 4 h (n = 8 mice) and 23 ± 4 units/ml at 25 h (n = 5 mice) after injection of BChE-IRDye 800CW. The BChE activity in the cerebellum, cerebrum, and brain stem of the animals treated with BChE/IRDye 800CW was 0.4–0.7 units/g, without significant difference among them. With confocal laser microscopy of the frozen brain sections prepared at 25 h after injection, the highest fluorescent signal levels were observed in the tissues surrounding the ventricles, cortex, and dentate gyrus, and lower signal levels were observed in the striatum and other hippocampal regions.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Patocka J., Kuca K., Jun D. (2004). Acetylcholinesterase and butyrylcholinesterase--important enzymes of human body. Acta Medica (Hradec Kralove).
2 Chiou S.Y., Huang C.F., Hwang M.T., Lin G. (2009). Comparison of active sites of butyrylcholinesterase and acetylcholinesterase based on inhibition by geometric isomers of benzene-di-N-substituted carbamates. J Biochem Mol Toxicol.
3 Goodall R. (2004). Cholinesterase: phenotyping and genotyping. Ann Clin Biochem.
4 Primo-Parmo S.L., Bartels C.F., Wiersema B., van der Spek A.F., Innis J.W., La Du B.N. (1996). Characterization of 12 silent alleles of the human butyrylcholinesterase (BCHE) gene. Am J Hum Genet.
5 Li B., Duysen E.G., Saunders T.L., Lockridge O. (2006). Production of the butyrylcholinesterase knockout mouse. J Mol Neurosci.
6 Geula C., Darvesh S. (2004). Butyrylcholinesterase, cholinergic neurotransmission and the pathology of Alzheimer's disease. Drugs Today (Barc).
7 Pepeu G., Giovannini M.G. (2009). Cholinesterase inhibitors and beyond. Curr Alzheimer Res.
8 Soreq H., Zakut H. (1990). Amplification of butyrylcholinesterase and acetylcholinesterase genes in normal and tumor tissues: putative relationship to organophosphorous poisoning. Pharm Res.
9 Kikuchi T., Zhang M.R., Ikota N., Fukushi K., Okamura T., Suzuki K., Arano Y., Irie T. (2004). N-[18F]fluoroethylpiperidin-4-ylmethyl butyrate: a novel radiotracer for quantifying brain butyrylcholinesterase activity by positron emission tomography. Bioorg Med Chem Lett.
10 Fukuda H., Okamura N. (2007). Brain Nerve.
11 Roivainen A., Rinne J., Virta J., Jarvenpaa T., Salomaki S., Yu M., Nagren K. (2004). Biodistribution and blood metabolism of 1-11C-methyl-4-piperidinyl n-butyrate in humans: an imaging agent for in vivo assessment of butyrylcholinesterase activity with PET. J Nucl Med.
12 Virta J.R., Tolvanen T., Nagren K., Bruck A., Roivainen A., Rinne J.O. (2008). 1-11C-methyl-4-piperidinyl-N-butyrate radiation dosimetry in humans by dynamic organ-specific evaluation. J Nucl Med.
13 Johnson N.D., Duysen E.G., Lockridge O. (2009). Intrathecal delivery of fluorescent labeled butyrylcholinesterase to the brains of butyrylcholinesterase knock-out mice: visualization and quantification of enzyme distribution in the brain. Neurotoxicology.
14 Duysen E.G., Lockridge O. (2008). Whole body and tissue imaging of the butyrylcholinesterase knockout mouse injected with near infrared dye labeled butyrylcholinesterase. Chem Biol Interact.
15 Duysen E.G., Li B., Lockridge O. (2009). The butyrylcholinesterase knockout mouse a research tool in the study of drug sensitivity, bio-distribution, obesity and Alzheimer's disease. Expert Opin Drug Metab Toxicol.
16 Li B., Duysen E.G., Lockridge O. (2008). The butyrylcholinesterase knockout mouse is obese on a high-fat diet. Chem Biol Interact.